# ^68^Ga-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-Tyr-cyclo(DAB-Arg-cyclo(Cys-Phe-D-Trp-Lys-Thr-Cys))

Chemical name: | ^68^Ga-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-Tyr-cyclo(DAB-Arg-cyclo(Cys-Phe-D-Trp-Lys-Thr-Cys))
Abbreviated name: | ^68^Ga-AM3
Synonym:
Agent Category: | Peptides
Target: | Somatostatin receptors (SSTRs)
Target Category: | Receptors
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | For structures of octreotide analogues, click on PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance?term=octreotide).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=somatostatin+receptor+and+targeted)]

The ^68^Ga-labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA)-Tyr-cyclo(DAB-Arg-cyclo(Cys-Phe-D-Trp-Lys-Thr-Cys)), abbreviated as ^68^Ga-AM3, is a somatostatin (SST)-based, bicyclic peptide conjugate developed by Fani et al. for SST receptor (SSTR)–targeted imaging of neuroendocrine tumors (1).

The human SSTR family is a group of G-protein–coupled receptors with five members (SSTR1–SSTR5). All receptor members have seven α-helical transmembrane domains and possess a highly conserved sequence motif (YANSCANPI/VLY) in the seventh topology, which serves as a signature sequence for this family (2-4). Overall, there is 39%–57% sequence identity among the members, with the highest homology between SSTR1 and SSTR4, and among SSTR2, SSTR3, and SSTR5, respectively. The two groups of receptors also differ in their interactions with SST and its analogs (3-6). SSTR2, SSTR3, and SSTR5 have a high affinity for octreotide and seglitide, whereas SSTR1 and SSTR4 exhibit a very low affinity for them. With the exception of SSTR2, the precise contributions of other members remain to be elucidated. This is largely due to the lack of highly selective ligands and the co-expression of different members in single cells. SSTRs are distributed widely in cells both in the nervous system and periphery, and they have been shown to be overexpressed in a large number of malignancies, with particularly high density in neuroendocrine tumors (2, 7, 8).

As the targets of SST radiopharmaceuticals, SSTRs are of considerable clinical relevance for tumor imaging and radionuclide therapy (2, 9, 10). Because the native SST has a very short biological half-life (<2 min), various analogs have been synthesized, including a group of bicyclic peptides. Bicyclic peptides were first synthesized to understand the bioactive conformation and pharmacophoric amino acid sequence, and to increase the metabolic stability of the natural peptide SST-14 (also known as somatotropin release-inhibiting factor (SRIF)-14) by increasing the rigidity of bicyclic peptides (11, 12). Thereafter, various modified bicyclic peptides have been synthesized and have exhibited higher potency and longer duration of biological activity than SRIF-14 (1, 11, 12). As seen in the structure of the lead peptide cyclo(Aha,cyclo(Cys-Phe-D-Trp-Lys-Thr-Cys)), conformational constraints are introduced by head-to-tail coupling of a 16-atom ring with 7-aminoheptanoic acid (Aha) to the N- and C-terminally amino acid–deleted octreotide. To identify metabolically stable pansomatostatin analogs, a group of investigators from Switzerland have generated a set of bicyclic peptides by forming a second 16-atom ring with Arg and γ-aminobutyric acid (GABA) while keeping the octreotide 20-atom sequence as an inner circle (13-15). These modifications led to the development of another lead peptide, cyclo(Arg-cyclo(Cys-Phe-D-Trp-Lys-Thr-Cys)-GABA), which is named HR3005 (1). Arg has been shown to be important for broad binding to SSTR subtypes, and GABA can be exchanged with diaminobutyric acid (DAB) for chelator coupling. Based on the HR3005 sequence, four bicyclic analogs have been further synthesized by Fani et al. from the same group (1). The influence of the conformational constraints on receptor binding profiles and the pharmacokinetics of the respective radiopeptides have been investigated. Studies by Fani et al. have shown that the high rigidity of these bicyclic radiopeptides leads to agonistic ligands with good affinity for all five SSTRs (1). The pharmacokinetic data of the DOTA-conjugated bicyclic peptide AM3 (DOTA-Tyr-cyclo(DAB-Arg-cyclo(Cys-Phe-D-Trp-Lys-Thr-Cys))) make it an excellent candidate for use as an imaging radiotracer (1).

### Related Resource Links:

- MICAD chapters on SSTR imaging (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=somatostatin+receptor+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information on SSTRs (http://www.ncbi.nlm.nih.gov/gene/?term=somatostatin+receptors)
- Articles on SSTRs in Online Mendelian Inheritance in Man (OMIM (http://www.ncbi.nlm.nih.gov/omim?term=somatostatin%20receptors))
- Somatostatin analogs in PubChem (http://www.ncbi.nlm.nih.gov/sites/entrez?db=pccompound&term=somatostatin)
- Bioassays of SSTRs in PubChem (http://www.ncbi.nlm.nih.gov/pcassay?term=somatostatin%20receptors)
- SSTR-related clinical trials in ClinicalTrial.gov (http://clinicaltrials.gov/ct2/results?term=somatostatin+receptors)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20956465)]

Fani et al. synthesized AM3 on the basis of the lead peptide of HR3005 (1). The GABA in HR3005 was replaced with DAB, followed by coupling of the peptide with DOTA through Tyr as a spacer. The ^68^Ga-labeled AM3 (^68^Ga-AM3) was prepared according to the method of Zhernosekov et al. (16). The radiotracer solution was prepared by dilution with 0.9% NaCl containing 0.1% bovine serum albumin. The overall yield was ~30%. The ^68^Ga-labeling yield was >97% with a specific activity of 35 GBq/µmol (0.95 Ci/µmol). The radiochemical purity of ^68^Ga-AM3 was >95%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20956465)]

Fani et al. characterized AM3 and ^68^Ga-AM3 for their binding affinity, cell internalization, and effect on intracellular Ca^2+^ release (1).

The binding profile of AM3 was determined with receptor autoradiography. The cell membrane pellets were prepared from human embryonic kidney (HEK) cells expressing different subtypes of SSTRs (17). The binding affinity was expressed as 50% inhibitory concentration (IC_50_; n > 3). The lead peptide HR3005 showed high affinity (comparable to SRIF-28) for SSTR2 (2.4 ± 0.6 nM) and SSTR3 (3.4 ± 0.8 nM), and moderate affinity for SSTR5 (14.5 ± 4.5 nM), SSTR1 (34 ± 10 nM), and SSTR4 (68 ± 22 nM), conferring almost pansomatostatin potency to this peptide. Replacement of GABA with DAB in the HR3005 did not change the affinity profile, whereas DOTA-coupling led to marked loss of affinity for all SSTR subtypes. By introducing Tyr as a spacer between DOTA and the peptide, the affinity of generated AM3 recovered to levels comparable to those of HR3005. The IC_50_ values of AM3 were 119 ± 6 nM for SSTR1, 2.3 ± 0.2 nM for SSTR2, 4.0 ± 0.03 nM for SSTR3, 97 ± 21 nM for SSTR4, and 27 ± 1 nM for SSTR5. The binding profile of ^68^Ga-AM3 was not examined.

The immunofluorescence microscopy–based internalization assay for SSTR2 and SSTR3 with HEK-SSTR2 and HEK-SSTR3 cells showed that AM3 elicited a pronounced relocation of SSTR2 and SSTR3 from the plasma membrane to the cytoplasm at 30 min after it was applied to the cells, an effect similar to that of the control, SRIF-28.

The stimulating effect of AM3 on the intracellular Ca^2+^ release was tested with HEK cells expressing SSTR2, SSTR3, and SSTR5. Intracellular Ca^2+^ release is a part of the signaling pathway regulated by native SST. On SSTR3 and SSTR5, no signal was found. On SSTR2, a large, concentration-dependent increase of the signal was observed. This indicates that AM3 is an agonist because of its stimulating effect on the Ca^2+^ release and high potencies similar to those of SRIF-14. The agonist-elicited response in terms of the half maximal effective concentration value was 21.5 ± 3.5 nM.

The internalization rate and efflux of ^177^Lu-AM3 were studied in HEK-SSTR2 and HEK-SSTR3 cells (for details, refer to the chapter on ^177^Lu-AM3 in MICAD (http://www.ncbi.nlm.nih.gov/books/NBK5330/)). Similar experiments were not performed for ^68^Ga-AM3. ^177^Lu-AM3 was extremely stable in human blood and serum at 37°C. However, the stability of ^68^Ga-AM3 was not tested.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20956465)]

Five-week-old athymic female Swiss nude mice with HEK-SSTR2 tumors (n = 4–7 mice/group) were used for biodistribution studies after injection of ^68^Ga-AM3 (100 µl/10 pmol per 0.4 MBq (0.011 mCi)) into the tail vein (1). Nonspecific uptake was determined with co-injection of 2,000-fold excess DOTANOC (18, 19). One group of mice was pre-injected with lysine 10 min before the injection of ^68^Ga-AM3 to study kidney blocking. The results were expressed as percentage of injected dose per gram of tissue (% ID/g).

The biodistribution profile of ^68^Ga-AM3 at early times was similar to that of ^177^Lu-AM3, showing fast blood clearance, fast nontarget clearance, and high receptor-mediated uptake in the tumors. At 1 h after injection, the SSTR2 tumors accumulated the highest ^68^Ga-AM3, with an uptake value of 11.92 ± 1.22% ID/g and a tumor/kidney ratio of 1.2. Blocking experiments with DOTANOC (high affinities for SSTR2, SSTR3, and SSTR5) confirmed the receptor-mediated uptake. Pre-injection of lysine (20 mg/100 µl) resulted in ~50% reduction of the kidney uptake with no significant impact on the tumor uptake.For PET/CT studies, the mice bearing HEK-SSTR2 tumors were injected with ^68^Ga-AM3, including a group preinjected with lysine and a group co-injected with DOTANOC (1). The mice were euthanized at 1 h after injection and scanned for 60 min using a routine combined PET/CT scanner. The images clearly showed high tumor and kidney uptake but negligible background. Preinjection of lysine resulted in a significant reduction of the kidney uptake. The specific uptake of ^68^Ga-AM3 was also confirmed using DOTANOC as a blocking agent, with which only the kidneys were visualized. The imaging study results were consistent with the biodistribution data.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Fani M., Mueller A., Tamma M.L., Nicolas G., Rink H.R., Cescato R., Reubi J.C., Maecke H.R. (2010). Radiolabeled bicyclic somatostatin-based analogs: a novel class of potential radiotracers for SPECT/PET of neuroendocrine tumors. J Nucl Med.
2 Froidevaux S., Eberle A.N. (2002). Somatostatin analogs and radiopeptides in cancer therapy. Biopolymers.
3 Tulipano G., Schulz S. (2007). Novel insights in somatostatin receptor physiology. Eur J Endocrinol.
4 van der Hoek J., Hofland L.J., Lamberts S.W. (2005). Novel subtype specific and universal somatostatin analogues: clinical potential and pitfalls. Curr Pharm Des.
5 Lesche S., Lehmann D., Nagel F., Schmid H.A., Schulz S. (2009). Differential effects of octreotide and pasireotide on somatostatin receptor internalization and trafficking in vitro. J Clin Endocrinol Metab.
6 Yim C.B., Dijkgraaf I., Merkx R., Versluis C., Eek A., Mulder G.E., Rijkers D.T., Boerman O.C., Liskamp R.M. (2010). Synthesis of DOTA-conjugated multimeric [Tyr3]octreotide peptides via a combination of Cu(I)-catalyzed "click" cycloaddition and thio acid/sulfonyl azide "sulfo-click" amidation and their in vivo evaluation. J Med Chem.
7 Strowski M.Z., Blake A.D. (2008). Function and expression of somatostatin receptors of the endocrine pancreas. Mol Cell Endocrinol.
8 Kwekkeboom D.J., Kam B.L., van Essen M., Teunissen J.J., van Eijck C.H., Valkema R., de Jong M., de Herder W.W., Krenning E.P. (2010). Somatostatin-receptor-based imaging and therapy of gastroenteropancreatic neuroendocrine tumors. Endocr Relat Cancer.
9 Bal C.S., Gupta S.K., Zaknun J.J. (2010). Radiolabeled somatostatin analogs for radionuclide imaging and therapy in patients with gastroenteropancreatic neuroendocrine tumors. Trop Gastroenterol.
10 de Jong M., Breeman W.A., Kwekkeboom D.J., Valkema R., Krenning E.P. (2009). Tumor imaging and therapy using radiolabeled somatostatin analogues. Acc Chem Res.
11 Veber D.F., Holly F.W., Paleveda W.J., Nutt R.F., Bergstrand S.J., Torchiana M., Glitzer M.S., Saperstein R., Hirschmann R. (1978). Conformationally restricted bicyclic analogs of somatostatin. Proc Natl Acad Sci U S A.
12 Veber D.F., Freidlinger R.M., Perlow D.S., Paleveda W.J., Holly F.W., Strachan R.G., Nutt R.F., Arison B.H., Homnick C., Randall W.C., Glitzer M.S., Saperstein R., Hirschmann R. (1981). A potent cyclic hexapeptide analogue of somatostatin. Nature.
13 Ginj M., Hinni K., Tschumi S., Schulz S., Maecke H.R. (2005). Trifunctional somatostatin-based derivatives designed for targeted radiotherapy using auger electron emitters. J Nucl Med.
14 Ginj M., Schmitt J.S., Chen J., Waser B., Reubi J.C., de Jong M., Schulz S., Maecke H.R. (2006). Design, synthesis, and biological evaluation of somatostatin-based radiopeptides. Chem Biol.
15 Ginj M., Zhang H., Waser B., Cescato R., Wild D., Wang X., Erchegyi J., Rivier J., Macke H.R., Reubi J.C. (2006). Radiolabeled somatostatin receptor antagonists are preferable to agonists for in vivo peptide receptor targeting of tumors. Proc Natl Acad Sci U S A.
16 Zhernosekov K.P., Filosofov D.V., Baum R.P., Aschoff P., Bihl H., Razbash A.A., Jahn M., Jennewein M., Rosch F. (2007). Processing of generator-produced 68Ga for medical application. J Nucl Med.
17 Reubi J.C., Schar J.C., Waser B., Wenger S., Heppeler A., Schmitt J.S., Macke H.R. (2000). Affinity profiles for human somatostatin receptor subtypes SST1-SST5 of somatostatin radiotracers selected for scintigraphic and radiotherapeutic use. Eur J Nucl Med.
18 Wild D., Schmitt J.S., Ginj M., Macke H.R., Bernard B.F., Krenning E., De Jong M., Wenger S., Reubi J.C. (2003). DOTA-NOC, a high-affinity ligand of somatostatin receptor subtypes 2, 3 and 5 for labelling with various radiometals. Eur J Nucl Med Mol Imaging.
19 Wild D., Macke H.R., Waser B., Reubi J.C., Ginj M., Rasch H., Muller-Brand J., Hofmann M. (2005). 68Ga-DOTANOC: a first compound for PET imaging with high affinity for somatostatin receptor subtypes 2 and 5. Eur J Nucl Med Mol Imaging.